# (-)-3-(4-Chlorophenyl)-N'-[(4-[^11^C]cyanophenyl)sulfonyl]-4-phenyl-4,5-dihydro-1H-pyrazole-1-carboxamidine

Chemical name: | (-)-3-(4-Chlorophenyl)-N'-[(4-[^11^C]cyanophenyl)sulfonyl]-4-phenyl- 4,5-dihydro-1H-pyrazole-1-carboxamidine
Abbreviated name: | [^11^C]CB1-(-)-12a
Synonym:
Agent category: | Compound
Target: | Cannabinoid CB1 receptors
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and some peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominantly in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. The CB2 receptors are present mainly on immune cells to modulate cytokine release. Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (4-6).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid that is found in marijuana and activates CB1 receptors (7). THC has a very high lipophilicity (log D_7.4_ value of 7), which causes imaging studies using radiolabeled THC to be unsuccessful because of slow entry into the brain and high nonspecific binding in the brain. However, a high lipophilicity is essential for binding to CB1 receptors, and an optimal lipophilicity (log D_7.4_ 1–4) is required for crossing the blood–brain barrier (BBB). Existing radiolabeled ligands are mainly analogs of the antagonist rimonabant (SR141716A) and the agonist WIN 55,212-2, which also exhibit high nonspecific binding and lipophilicity, limiting their application in imaging (8). Therefore, there is a need to lower the lipophilicity of the CB1 radioligands with little effect on binding affinity and ability to cross the BBB. (-)-3-(4-chlorophenyl)-N'-[(4-[^11^C]cyanophenyl)sulfonyl]-4-phenyl- 4,5-dihydro-1H-pyrazole-1-carboxamidine ([^11^C]CB1-(-)-12a) is a potent and selective CB1 antagonist with nanomolar affinity and lower lipophilicity than SR141716A (9). [^11^C]CB1-(-)-12a is being developed as a positron emission tomography (PET) agent for the non-invasive study of CB1 receptors in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20synthesis)]

Donohue et al. (9) reported synthesis of [^11^C]CB1-(+/-)-12a by reaction of the bromo precursor (-)-3-(4-chlorophenyl)-N'-[(4-bromophenyl)sulfonyl]-4-phenyl- 4,5-dihydro-1H-pyrazole-1-carboxamidine with [^11^C]HCN in DMSO in the presence of KOH, Pd(PPh_3_)_4_ and K2.2.2 at 135°C for 5 min. An average radiochemical yield was 36% with a total synthesis time of 30 min after purification by high-performance liquid chromatography. The specific activity was 56 GBq/μmol (1.51 Ci/μmol; n = 2) at the end of synthesis with a radiochemical purity of >97%. Using NaHCO_3_ instead of KOH gave [^11^C]CB1-(-)-12a to [^11^C]CB1-(+)-12a in a 9:1 ratio. Using the (+)-iodo precursor and KH_2_PO_4_ gave [^11^C]CB1-(+)-12a to [^11^C]CB1-(-)-12a in a 9.7: 0.3 ratio. [^11^C]CB1-(+)-12a and [^11^C]CB1-(-)-12a were obtained in >94% chiral purity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20in%20vitro)]

Donohue et al. (9) reported that CB1-(-)-12a had inhibition constant (K_i_) values of 0.5 ± 0.1 nM for CB1 and >5,000 nM for CB2. [^11^C]CB1-(+)-12a showed K_i_ values of 16.9 ± 2.0 nM for CB1 and >5,000 nM for CB2. Each enantiomer exhibited a Clog D_7.4_ (lipophilicity) value of 3.85.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20%28primate%20not%20human%29)]

Donohue et al. (9) performed a biodistribution PET study in two anesthetized cynomolgus monkeys injected with [^11^C]CB1-(+/-)-12a, which showed a rapid accumulation of radioactivity in the brain. Selective maximal uptake was observed in the striatum, followed by the cortex, cerebellum, thalamus and pons. The thalamus and pons exhibited lower binding than the other brain regions. The peak level of 220% standardized uptake value (SUV) was reached in the striatum at 30 min after injection and decreased to 180% SUV at 90 min. The lowest peak accumulation was in the pons with 150% SUV at 30 min and 124% SUV at 90 min. Administration of a high potency cannabinoid subtype-1 receptor ligand, N-(4-fluoro-benzyl)-4-(3-(piperidin-1-yl)-indole-1-sulfonyl)benzamide (PipISB), 20 min before or 25 min after tracer injection reduced the radioactivity in the brain to homogeneity with 85% SUV and 95% SUV at 90 min, respectively. Injection of the higher affinity enantiomer [^11^C]CB1-(-)-12a exhibited a similar accumulation pattern in the brain as [^11^C]CB1-(+/-)-12a. On the other hand, injection of the lower affinity enantiomer [^11^C]CB1-(+)-12a showed the peak brain accumulation was 280% SUV at 1.5 min and decreased to 95% SUV at 90 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CB1%2012a%20and%20human)]

No publication is currently available.

## NIH Support

Intramural research program

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
5 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
6 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
7 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
8 Gifford A.N., Makriyannis A., Volkow N.D., Gatley S.J. (2002). In vivo imaging of the brain cannabinoid receptor. Chem Phys Lipids.
9 Donohue S.R., Pike V.W., Finnema S.J., Truong P., Andersson J., Gulyas B., Halldin C. (2008). Discovery and labeling of high-affinity 3,4-diarylpyrazolines as candidate radioligands for in vivo imaging of cannabinoid subtype-1 (CB1) receptors. J Med Chem.